# ^99m^Tc(CO)_3_-Anti-carcinoembryonic antigen (CEA) humanized CEA5 graft nanobody

Chemical name: | ^99m^Tc(CO)_3_-Anti-carcinoembryonic antigen antigen (CEA) humanized CEA5 graft nanobody
Abbreviated name: | ^99m^Tc-Humanized CEA5 graft
Synonym:
Agent category: | Antibody fragment, humanized nanobody
Target: | Carcinoembryonic antigen (CEA)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=180211), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=29856) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=5670) for more information about CEA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CEA%20nanobody%20)]

Carcinoembryonic antigen (CEA) was first identified from extracts of human colon adenocarcinoma (1) and fetal gut (2). CEA is a β-glycoprotein, and its predominant expression on the cell surface is increased in a variety of carcinomas and in certain inflammatory conditions, such as inflammatory bowel disease (3, 4). CEA has a molecular weight of ~180 kDa, and it can be shed and detected in serum (5). CEA expression is observed in patients with various carcinomas of the colon, lung, thyroid, uterus, ovary, pancreas, and medullary thyroid. Radiolabeled monoclonal antibodies (mAbs) have been developed for both the diagnosis and treatment of tumors (6, 7). However, the pharmacokinetics of intact radiolabeled mAbs, with high liver uptake and slow blood elimination, are generally not ideal for imaging (8, 9). Smaller antibody fragments, such as scFv, Fab, or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. Nanobodies are the smallest intact antigen-binding fragments (15 kDa) isolated from heavy-chain camelid antibodies with efficient and specific tumor targeting (10-12). Anti-CEA nanobody CEA5 (NbCEA5, also known as cAb-CEA5) exhibits high binding affinity to CEA (K_d_, 0.34 nM) (13). In order to minimize immunogenicity of nanobodies in humans, the antigen-binding loops of NbCEA5 were genetically grafted onto the framework of a humanized nanobody scaffold (h-NBBcII10_FGLA_) to form humanized CEA5 graft nanobody (14). The three nanobodies (NbCEA5, humanized nanobody scaffold, and humanized CEA5 graft) were radiolabeled with ^99m^Tc using tricarbonyl chemistry for noninvasive in vivo single-photon emission computed tomography (SPECT) imaging of CEA expression in tumors in mice.

### Related Resource Links:

- Chapters in MICAD (CEA (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=CEA+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), nanobody (http://www.ncbi.nlm.nih.gov/books?term=nanobody%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (CEA (http://www.ncbi.nlm.nih.gov/gene/1048))
- Articles in Online Mendelian Inheritance in Man (OMIM) (CEA (http://www.ncbi.nlm.nih.gov/omim/114890))
- Clinical trials (CEA (http://www.clinicaltrials.gov/ct2/results?term=Carcinoembryonic+antigen&pg=2), nanobody (http://www.clinicaltrials.gov/ct2/results?term=nanobody))
- Drug information in FDA (CEA (http://google2.fda.gov/search?q=Carcinoembryonic+antigen&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CEA%20nanobody%20and%20synthesis)]

NbCEA5, humanized nanobody scaffold, and humanized CEA5 graft were produced as hexahistidine-tagged proteins in Escherichia coli (14). A solution of [^99m^Tc(H_2_O)_3_(CO)_3_]^+^ and nanobodies was incubated for 90 min at 52°C. ^99m^Tc-Labeled nanobodies were isolated with column chromatography, with a radiochemical purity of >99%. The specific activities, radiochemical yields, and stability of the ^99m^Tc-labeled nanobodies were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CEA%20nanobody%20and%20in%20vitro)]

Flow cytometry analysis showed that NbCEA5 and humanized CEA5 graft bound efficiently to CEA-expressing CHO and human colon adenocarcinoma LS174T cells but not to CEA-negative CHO cells (14). Humanized nanobody scaffold exhibited no binding to either CHO cell types. Binding experiments with the use of a Biacore sensor chip immobilized with CEA protein showed that the K_d_ values of NbCEA5, humanized nanobody scaffold, and humanized CEA5 graft were 0.34 nM, >10 µM, and 9.88 nM, respectively. ^99m^Tc-NbCEA5 and ^99m^Tc-humanized CEA5 graft exhibited efficient binding to both purified CEA protein and CEA-expressing CHO cells, whereas ^99m^Tc-humanized nanobody scaffold exhibited little binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CEA%20nanobody%20and%20rodentia)]

Vaneycken et al. (14) performed SPECT imaging analysis in nude mice (n = 6) bearing LS174T tumors at 1 h after injection of 45–155 MBq (1.2–4.2 mCi, 0.17 nmol) ^99m^Tc-NbCEA5, ^99m^Tc- humanized CEA5 graft, or ^99m^Tc-humanized nanobody scaffold. Intense radioactivity levels were observed in the kidneys (>87% ID/cm^3^) and urinary bladder for all ^99m^Tc-nanobodies, which were cleared equally quickly from the blood. Accumulation levels in the liver, lung, and muscle were low (<3.1% ID/cm^3^). Radioactivity accumulation levels in the tumors for ^99m^Tc-NbCEA5, ^99m^Tc-humanized nanobody scaffold, and ^99m^Tc- humanized CEA5 graft were 7.09 ± 1.36%, 0.21 ± 0.05%, and 6.15 ± 2.33% ID/cm^3^. The tumor accumulation of ^99m^Tc- humanized CEA5 graft was not significantly different from that of ^99m^Tc-NbCEA5 (P = 0.40). The imaging studies were not confirmed with ex vivo biodistribution studies, and no blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CEA%20nanobody%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CEA%20nanobody%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CEA%20nanobody%20and%20human)]

No publication is currently available.

## References

1 Gold P., Freedman S.O. (1964). Demonstration of tumor-specific antigens in human colonic carcinomata by immunological tolerance and absorption techniques. The Journal of Experimental Medicine.
2 Krupey J., Gold P., Freedman S.O. (1967). Purification and characterization of carcinoembryonic antigens of the human digestive system. Nature.
3 Kowalsky, R.J., and S.W. Falen, Radiopharmaceuticals in nuclear pharmacy and nuclear medicine2004, American Pharmacists Association: Washington, D.C. p. 733-752.
4 Wahl R.L., Philpott G., Parker C.W. (1983). Monoclonal antibody radioimmunodetection of human-derived colon cancer. Invest Radiol.
5 Primus F.J., Freeman J.W., Goldenberg D.M. (1983). Immunological heterogeneity of carcinoembryonic antigen: purification from meconium of an antigen related to carcinoembryonic antigen. Cancer Res.
6 Kenanova V., Olafsen T., Crow D.M., Sundaresan G., Subbarayan M., Carter N.H., Ikle D.N., Yazaki P.J., Chatziioannou A.F., Gambhir S.S., Williams L.E., Shively J.E., Colcher D., Raubitschek A.A., Wu A.M. (2005). Tailoring the pharmacokinetics and positron emission tomography imaging properties of anti-carcinoembryonic antigen single-chain Fv-Fc antibody fragments. Cancer Res.
7 Wu A.M., Olafsen T. (2008). Antibodies for molecular imaging of cancer. Cancer J.
8 Olafsen T., Wu A.M. (2010). Antibody vectors for imaging. Semin Nucl Med.
9 Wu A.M. (2009). Antibodies and antimatter: the resurgence of immuno-PET. J Nucl Med.
10 Arbabi Ghahroudi M., Desmyter A., Wyns L., Hamers R., Muyldermans S. (1997). Selection and identification of single domain antibody fragments from camel heavy-chain antibodies. FEBS Lett.
11 Desmyter A., Decanniere K., Muyldermans S., Wyns L. (2001). Antigen specificity and high affinity binding provided by one single loop of a camel single-domain antibody. J Biol Chem.
12 Muyldermans S. (2001). Single domain camel antibodies: current status. J Biotechnol.
13 Cortez-Retamozo V., Backmann N., Senter P.D., Wernery U., De Baetselier P., Muyldermans S., Revets H. (2004). Efficient cancer therapy with a nanobody-based conjugate. Cancer Res.
14 Vaneycken I., Govaert J., Vincke C., Caveliers V., Lahoutte T., De Baetselier P., Raes G., Bossuyt A., Muyldermans S., Devoogdt N. (2010). In vitro analysis and in vivo tumor targeting of a humanized, grafted nanobody in mice using pinhole SPECT/micro-CT. J Nucl Med.